# 2-[2-[2-Chloro-3-[2-[1,3-dihydro-3,3-dimethyl-1-(4-sulfobutyl)-2H-indol-2-ylidene]-ethylidene]-1-cyclohexen-1-yl]-ethenyl]-3,3-dimethyl-1-(4-sulfobutyl)-3H-indolium

Chemical name: | 2-[2-[2-Chloro-3-[2-[1,3-dihydro-3,3-dimethyl-1-(4-sulfobutyl)-2H-indol-2-ylidene]-ethylidene]-1-cyclohexen-1-yl]-ethenyl]-3,3-dimethyl-1-(4-sulfobutyl)-3H-indolium
Abbreviated name: | IR-783
Synonym:
Agent category: | Compound
Target: | Lysosomes and mitochondria
Target category: | Unknown
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal: | IR-783
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IR-783)]

Optical fluorescence imaging is increasingly being used to monitor biological functions of specific targets (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the natural background fluorescence interference of biomolecules, which provides a high contrast between target and background tissues in small animals. NIR fluorophores have a wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. NIR fluorophores also have high sensitivity, attributable to low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components such as diode lasers and silicon detectors. NIR fluorescence imaging is a non-invasive complement to radionuclide imaging in small animals.

Among the various NIR agents, only indocyanine green (ICG), with absorption at 780 nm and emission at 820 nm, is approved by the United States Food and Drug Administration for clinical applications in angiography, blood flow evaluation, and liver function assessment (4). It is also under evaluation in several clinical trials (http://clinicaltrials.gov/ct2/results?term=indocyanine+green) for other applications. However, ICG has a plasma half-life of 2–4 min because it forms aggregates in the blood and is rapidly cleared from blood circulation (5). ICG is prone to photobleaching and non-specific quenching via its extensive binding to proteins. On the other hand, the fluorescence efficiency of some cyanine dyes can increase by ~1,000-fold upon binding to proteins and nucleic acids (6).

Organic anion transporters (OATPs) are responsible for the transport of a diverse group of substances (hormones, xenobiotics, and bile acids) (7). Some OATPs have been shown to be overexpressed in various human cancer tissues and cancer cell lines (8, 9). Lysosomes are membranous vesicles found in most mammalian cells (10). Lysosomes contain various types of proteases, which have been implicated in migration, invasion, and metastasis of malignant cancer cells by degradation of extracellular matrix (11). Lysosomes are found to be larger in malignant cancer cells than in benign cancer cells (12). 2-[2-[2-Chloro-3-[2-[1,3-dihydro-3,3-dimethyl-1-(4-sulfobutyl)-2H-indol-2-ylidene]-ethylidene]-1-cyclohexen-1-yl]-ethenyl]-3,3-dimethyl-1-(4-sulfobutyl)-3H-indolium (IR-783) has been shown to accumulate in the mitochondria and lysosomes of cancer cells (13). Uptake of IR-783 may be dependent upon OATPs. Yang et al. (13) have evaluated the usefulness of IR-783 as a probe for NIR imaging of tumors.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=IR-783+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (Organic anion transporters (http://www.ncbi.nlm.nih.gov/sites/gene?Db=gene&Cmd=DetailsSearch&Term=OATP%5BAll+Fields%5D)).
- Articles in OMIM (Organic anion transporters (http://www.ncbi.nlm.nih.gov/sites/omim?Db=omim&Cmd=DetailsSearch&Term=oatp%5BAll+Fields%5D))
- Clinical trials (Indocyanine green (http://www.clinicaltrials.gov/ct2/results?term=indocyanine+green))
- Drug information in FDA (Indocyanine green (http://google2.fda.gov/search?q=indocyanine+green&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=9&y=13))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IR-783+Synthesis)]

IR-783 is commercially available. IR-783 has an extinction of coefficient of 157,000 M^-1^cm^-1^ and a quantum yield of 0.11, with a maximal excitation wavelength of 768 nm and a maximal emission wavelength of 784 nm in saline (14). The fluorescence intensities at pH 3–5 were higher than those at pH 6.4–7.2.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IR-783+In+Vitro)]

Yang et al. (13) showed that 0.02 mM IR-783 exhibited a two-phase uptake in human prostate ARcAP_M_ tumor cells competed at 12 min and 30 min with minimal cell cytotoxicity in cultures. The measured fluorescence intensity correlated with the concentrations (0.001, 0.01, 0.02, and 0.05 mM) of IR-783 in ARcAP_M_ cells. In normal prostate epithelial cells, the uptake of IR-783 (0.02 mM) only began at 12 min with 3-fold lower signal intensity. The uptake in ARcAP_M_ cells was abolished with 0.25 mM bromosulfophthalein, a competitive inhibitor of OATPs. Most of the IR-783 signal was co-localized with the lysosomal and mitochondrial tracking dyes. IR-783 accumulated preferentially in a panel of human and mouse cancer cells versus normal tissues and cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IR-783+Rodentia)]

Yang et al. (13) performed studies of IR-783 (~10 nmol/mouse) in nude mice bearing subcutaneous human bladder tumors (T-24), subcutaneous pancreas tumors (MIA PaCa-2), orthotopic prostate tumors (ARCaP_M_), and kidney tumors (SN12C, intraosseously to tibia) using a whole-body fluorescence detection system. IR-783 showed a clear fluorescence signal in all four tumors at 24 h after injection with no background interference. IR-783 was also able to detect the primary tumors and metastatic tumors in two transgenic mouse models (TRAMP mouse model for prostate cancer and Apc^Min/+^ mouse model for colon cancer) with high degrees of tumor metastases. Histopathological analysis of all tumor sections confirmed uptake of IR-783 in tumor cells but not in normal cells. An ex vivo biodistribution study showed that the ARcAP_M_ tumor exhibited >5-fold greater fluorescence intensity than the liver, kidney, lung, heart, and spleen at 24 h after IR-783 injection (n = 3; P < 0.05). No blocking studies were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IR-783+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IR-783+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IR-783+human)]

No publication is currently available.

## NIH Support

P50 CA128301, U54 CA119338, R01 CA122602-02

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Sakka S.G. (2007). Indocyanine green plasma disappearance rate as an indicator of hepato-splanchnic ischemia during abdominal compartment syndrome. Anesth Analg.
5 Desmettre T., Devoisselle J.M., Mordon S. (2000). Fluorescence properties and metabolic features of indocyanine green (ICG) as related to angiography. Surv Ophthalmol.
6 Silva G.L., Ediz V., Yaron D., Armitage B.A. (2007). Experimental and computational investigation of unsymmetrical cyanine dyes: understanding torsionally responsive fluorogenic dyes. J Am Chem Soc.
7 Marzolini C., Tirona R.G., Kim R.B. (2004). Pharmacogenomics of the OATP and OAT families. Pharmacogenomics.
8 Lee W., Belkhiri A., Lockhart A.C., Merchant N., Glaeser H., Harris E.I., Washington M.K., Brunt E.M., Zaika A., Kim R.B., El-Rifai W. (2008). Overexpression of OATP1B3 confers apoptotic resistance in colon cancer. Cancer Res.
9 Muto M., Onogawa T., Suzuki T., Ishida T., Rikiyama T., Katayose Y., Ohuchi N., Sasano H., Abe T., Unno M. (2007). Human liver-specific organic anion transporter-2 is a potent prognostic factor for human breast carcinoma. Cancer Sci.
10 de Duve C. (2005). The lysosome turns fifty. Nat Cell Biol.
11 Mignatti P., Rifkin D.B. (1993). Biology and biochemistry of proteinases in tumor invasion. Physiol Rev.
12 Glunde K., Guggino S.E., Solaiyappan M., Pathak A.P., Ichikawa Y., Bhujwalla Z.M. (2003). Extracellular acidification alters lysosomal trafficking in human breast cancer cells. Neoplasia.
13 Yang X., Shi C., Tong R., Qian W., Zhau H.E., Wang R., Zhu G., Cheng J., Yang V.W., Cheng T., Henary M., Strekowski L., Chung L.W. (2010). Near IR heptamethine cyanine dye-mediated cancer imaging. Clin Cancer Res.
14 Li C., Greenwood T.R., Glunde K. (2008). Glucosamine-bound near-infrared fluorescent probes with lysosomal specificity for breast tumor imaging. Neoplasia.